# 2'-Fluoro-2'-deoxy-5'-[^123/124/125/131^I]iodo-1β-D-arabinofuranosyluracil

Chemical name: | 2'-Fluoro-2'-deoxy-5'-[^123/124/125/131^I]iodo-1β-D-arabinofuranosyluracil
Abbreviated name: | [^123/124/125/131^I]FIAU
Synonym:
Agent category: | Compound
Target: | Herpes simplex virus thymidine kinase (HSV-TK)
Target category: | Phosphorylation
Method of detection: | Positron emission tomography (PET)/ Single-photon emission computed tomography (SPECT)
Source of signal: | ^123/124/125/131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FIAU)]

A potential approach to the treatment of diseases and genetic disorders in humans is gene therapy [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22gene%20therapy%22%5BMeSH%20Terms%5D%20OR%20Gene%20Therapy%5BText%20Word%5D)]. This is a technique whereby the absent or malfunctioned gene is replaced by a working gene to produce an enzyme or protein to correct the progression of the disease. Noninvasive molecular imaging technologies play an important role in the fields of gene therapy by monitoring gene expression continuously in living animals (1). Magnetic resonance imaging (MRI), optical imaging, ultrasound imaging, and radionuclide imaging (positron emission tomography (PET)/single photon emission computed tomography (SPECT)) modalities have been applied for gene therapy of cancer as well as cardiovascular, neurological, musculoskeletal, hepatic, immunological, diabetic, and inherited diseases in small animals (2-10). These noninvasive imaging technologies allow quantitative assessments of the magnitude, location, and duration of the transgene expression. Gene therapy can be achieved either ex vivo or in vivo. The gene can be delivered using a viral or nonviral vector, such as liposome and naked DNA. Retrovirus, adenovirus, adeno-associated virus, and herpes simplex virus have been used as gene transfer vectors. Imaging transgene expression can help to optimize gene therapy. There are two imaging strategies, direct and indirect. Direct imaging uses a target-specific probe directly to the target gene, such as receptor, enzyme, and antigen. For example, herpes simplex virus type 1 thymidine kinase (HSV1-tk) vector is transduced in cells first. Labeled FIAU is introduced later to monitor its expression. Indirect imaging involves coupling the target gene to a reporter gene, the expression of which can be tracked by a specific reporter gene probe. For example, the VEGF gene is linked with HSV1-tk in a vector, which is transduced in cells. Labeled FIAU is then introduced to monitor the expression of VEGF via the expression of the reporter (HSV1-tk).

Currently, there are two approaches to image transgene expression by using either a reporter enzyme using a substrate probe or a reporter receptor using a receptor ligand probe. The enzymes include cytosine deaminase, β-galactosidase, tyrosinase, and HSV1-tk. The Na^+^/Iˉ symporter (NIS) gene has been studied as a potential reporter gene as well as a therapeutic gene (11). The most extensively studied reporter enzyme gene is HSV1-tk (8, 12). The reporter receptors are dopamine D_2_ receptor (D_2_R) (13) and somatostatin receptor subtype-2 (hSSTR2) (14).

HSV1-tk is a commonly studied suicide gene for cancer therapy of glioma, prostate cancer, leukemia, and lymphoma (10, 15). Suicide gene therapy is based on the enzymatic conversion of a nontoxic prodrug into a lethal drug by a transgene. Anti-HSV nucleoside analogs, such as acyclovir, ganciclovir, and penciclovir, are converted to monophosphates by HSV-TK. The cellular enzymes then convert the monophosphates to di- and triphosphates, which inhibit mammalian DNA polymerase. HSV1-tk has also been widely studied as a reporter gene. The HSV prodrugs have been explored for HSV1-tk reporter gene imaging. The selective phosphorylation of the produg probes by HSV1-TK leads to trapping within the transduced cells and not significantly in the other cells. Many radiolabeled acycloguanosine and thymidine derivatives have been studied for HSV1-tk reporter gene imaging in vitro, in small animals, and in humans (16). 2'-Fluoro-2'-deoxy-5'-iodo-1β-D-arabinofuranosyluracil (FIAU) has been tested as an anti-viral thymidine nucleoside analog against herpes and hepatitis viruses. Radiolabeled FIAU has been evaluated in vitro and in small animals to be a potential imaging agent for HSV1-tk gene expression using PET/SPECT imaging (17, 18).

### Related Resource Links:

- Chapters in MICAD (HSV-TK (http://www.ncbi.nlm.nih.gov/books/?term=HSV-TK+AND+micad%5Bbook%5D))
- Gene information in NCBI (HSV-TK (http://www.ncbi.nlm.nih.gov/gene/2703374))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MC1R (http://omim.org/entry/155555))
- Clinical trials ([^124^I]FIAU (http://www.clinicaltrials.gov/ct2/results?term=FIAU&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FIAU%20AND%20iodine%20radioisotopes%29%20AND%20synthesis)]

2'-Fluoro-2'-deoxy-1-beta-D-arabinofuranosyluracil (FAU) was generally labeled by direct iodination with [*I]NaI to form [*I]FIAU (19, 20). [*I] denotes [^123^I], [^124^I], [^125^I], or [^131^I]. [^*^I]FIAU was isolated by column chromatography or high-performance liquid chromatography (HPLC) purification. Radiochemical yield was 51-55% with radiochemical purity of >97%. In an alternative approach, 5-trimethylstannyl-1-(2'-fluoro-2'deoxy-1-beta-D-arabinofuranosyl)uracil (FTAU) was reacted with [*I]NaI to form [*I]FIAU (21, 22). The radiochemical yield was in the range of 85-95% with radiochemical purity of >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iodine%20isotopes%20and%20FIAU%29%20AND%20in%20vitro)]

[^131^I]FIAU was stable in human serum and whole blood at 37ºC over a period of 24 h. The uptake of [^125^I]FIAU in D-247 human glioma cells in vitro was 20-fold greater than that of [^125^I]IUdR. The uptake was blocked by an excess of the respective unlabeled compounds. More than 80% of the cellular radioactivity was incorporated into DNA (22).

FIAU was shown to be greatly accumulated in various HSV1-tk transduced cell lines over control cells (17, 18, 21, 23). In general, FIAU accumulation was better than FHBG and FHPG (17, 20). The transduced cells were more sensitive to ganciclovir inhibition as compared to the control cells in vitro (18, 23). Highly significant relationships were observed between HSV1-tk expression and sensitivity to ganciclovir and FIAU accumulation in the transduced cell lines (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FIAU%20and%20iodine%20isotopes%29%20AND%20rodentia)]

Biodistribution of [^131^I]FIAU was studied in normal mice. The initial tracer uptake was high at 0.25 h in liver, kidneys, muscle, blood, and urine. The uptakes in most organs decreased with time with the exception of the thyroid, which showed an increasing uptake with time (22). Biodistribution studies of FIAU in mice and rats bearing HSV1-tk-positive and -negative tumors showed excellent tracer uptakes in the positive tumors within 1 h, which persisted up to 24 h (18, 20). Clear PET and SPECT images of the HSV1-tk-expressing tumors were observed.

Rats were percutaneously injected with similar titers of adenovirus-expressing HSV1-tk, HSV1-sr39tk, or control gene into the myocardium, followed by [^124^I]FIAU (HSV1-tk rats and controls) or [^18^F]FHBG (HSV1-sr39tk rats and controls) 2 days later (24). Dynamic PET was performed during the 2 h after injection of the tracer. A significant cardiac [^124^I]FIAU accumulation of 1.24-fold increase over controls occurred in images obtained early (10–30 min) after the tracer injection. However, no difference between HSV1-tk-infected animals and controls was seen in the images obtained later because of tracer washout. For [^18^F]FHBG, specific myocardial accumulation greater than background levels was detected in HSV1-sr39tk-infected animals at early imaging and increased over time until the latest imaging (105–120 min). At maximum, cardiac [^18^F]FHBG uptake showed a 4.15-fold increase compared with controls (105-120 min). Co-expression of the reporter gene HSV1-tk and a therapeutic gene is opening up more opportunities for gene therapy of heart diseases (5).

In another study, RG2 rat glioma tumor cells were transduced with HSV1-tk and transplanted subcutaneously in nude rats (20). The in vitro and in vivo imaging results show that [^124^I]FIAU is a better reporter probe than [^18^F]FHBG for imaging HSV1-tk expression, with greater sensitivity and higher accumulation at 2 and 24 h. Therefore, different cell types may handle reporter gene and reporter probe differently.

Various preclinical studies showed that [^124^I]FIAU can be used to monitor co-expression of HSV1-tk and a cis-linked transgene in mice and rats (25-28). This approach will facilitate further development of gene-therapy protocols in humans. [^124^I]FIAU was reported to be a useful agent to image bacterial infections (29) and tumor-localized bacteria expressing HSV1-tk in small animals (30).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FIAU%20and%20iodine%20isotopes%29%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

In cats, the kinetic analysis of [^124^I]FIAU radioactivity showed an early peak (1-2 min after injection) in heart and kidneys (0.20% injected dose (ID)/g; SUV, 4.0), followed by a second peak (10-20 min after injection) in liver and spleen (0.16% ID/g; SUV, 3.2) (19). Subsequent clearance from tissues and a late peak in the bladder were observed at 10-15 h after injection. In the unlesioned cat brain, no substantial [^124^I]FIAU uptake occurred throughout the PET measurements (0.02% ID/g; SUV, 0.4), indicating that FIAU cannot cross the intact blood-brain barrier (BBB).

Bengel et al. (31) reported that PET imaging of HSV1-tk expression with [^124^I]FIAU in pig hearts was limited to the first 30 min because of a rapid washout of [^124^I]FIAU from the hearts. However, Miyagawa et al. (24) showed that good images were obtained with [^18^F]FHBG in HSV1-sr39tk-expressing rat and pig hearts up to 120 min but not with [^124^I]FIAU in HSV1-tk-expressing hearts.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28FIAU%20and%20iodine%20isotopes%29AND%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iodine%20isotopes%20and%20FIAU%29%20and%20humans%20not%20cell%20line)]

In one recurrent glioblastoma patient, [^124^I]FIAU uptake in normal brain was very low (0.0002%ID/g; SUV, 0.16) after a bolus injection of 77.7 MBq or 2.1 mCi [^124^I]FIAU (19). In contrast, the recurrent glioblastoma showed relatively high uptake of radioactivity (5-10 min after injection; 0.001%ID/g; SUV, 0.8), which was cleared slowly over the 68-h imaging period. The presence of the tumor was confirmed by MRI, [^11^C]MET and [^18^F]FDG measurements. However, substantial uptake of [^124^I]FIAU may occur within areas of BBB disruption (e.g., glioblastoma), which is helpful for imaging clinically relevant levels of HSV1-tk gene expression in brain tumors after gene therapy.

HSV1-tk liposomal vector was infused intratumorally to five recurrent glioblastoma patients, followed by ganciclovir treatment for 14 days (32). Treatment responses were measured by MRI, [^11^C]MET PET and [^18^F]FDG PET as well as [^124^I]FIAU PET. One of five patients showed specific uptake of [^124^I]FIAU with signs of necrosis as observed by [^11^C]MET and [^18^F]FDG radioactivity within the volume of specific [^124^I]FIAU trapping after ganciclovir treatment. The other four patients with no specific [^124^I]FIAU uptake may be explained by their significantly lower number of proliferating tumor cells per voxel and therefore inefficient transfer of the HSV1-tk gene. [^124^I]FIAU PET imaging of HSV1-tk gene expression in patients is feasible and that the gene expression may predict the therapeutic effect.

## References

1 Gambhir S.S., Herschman H.R., Cherry S.R., Barrio J.R., Satyamurthy N., Toyokuni T., Phelps M.E., Larson S.M., Balatoni J., Finn R., Sadelain M., Tjuvajev J., Blasberg R. (2000). Imaging transgene expression with radionuclide imaging technologies. Neoplasia.
2 Herschman H.R. (2004). PET reporter genes for noninvasive imaging of gene therapy, cell tracking and transgenic analysis. Crit Rev Oncol Hematol.
3 Hildebrandt I.J., Gambhir S.S. (2004). Molecular imaging applications for immunology. Clin Immunol.
4 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
5 Min J.J., Gambhir S.S. (2004). Gene therapy progress and prospects: noninvasive imaging of gene therapy in living subjects. Gene Ther.
6 Prieto J., Qian C., Hernandez-Alcoceba R., Gonzalez-Aseguinolaza G., Mazzolini G., Sangro B., Kramer M.G. (2004). Gene therapy of liver diseases. Expert Opin Biol Ther.
7 Shah K., Jacobs A., Breakefield X.O., Weissleder R. (2004). Molecular imaging of gene therapy for cancer. Gene Ther.
8 Tjuvajev J.G., Stockhammer G., Desai R., Uehara H., Watanabe K., Gansbacher B., Blasberg R.G. (1995). Imaging the expression of transfected genes in vivo. Cancer Res.
9 Wu J.C., Tseng J.R., Gambhir S.S. (2004). Molecular imaging of cardiovascular gene products. J Nucl Cardiol.
10 Yechoor V., Chan L. (2005). Gene therapy progress and prospects: gene therapy for diabetes mellitus. Gene Ther.
11 Dadachova E., Carrasco N. (2004). The Na/I symporter (NIS): imaging and therapeutic applications. Semin Nucl Med.
12 Gambhir S.S., Barrio J.R., Wu L., Iyer M., Namavari M., Satyamurthy N., Bauer E., Parrish C., MacLaren D.C., Borghei A.R., Green L.A., Sharfstein S., Berk A.J., Cherry S.R., Phelps M.E., Herschman H.R. (1998). Imaging of adenoviral-directed herpes simplex virus type 1 thymidine kinase reporter gene expression in mice with radiolabeled ganciclovir. J Nucl Med.
13 MacLaren D.C., Gambhir S.S., Satyamurthy N., Barrio J.R., Sharfstein S., Toyokuni T., Wu L., Berk A.J., Cherry S.R., Phelps M.E., Herschman H.R. (1999). Repetitive, non-invasive imaging of the dopamine D2 receptor as a reporter gene in living animals. Gene Ther.
14 Zinn K.R., Buchsbaum D.J., Chaudhuri T.R., Mountz J.M., Grizzle W.E., Rogers B.E. (2000). Noninvasive monitoring of gene transfer using a reporter receptor imaged with a high-affinity peptide radiolabeled with 99mTc or 188Re. J Nucl Med.
15 Yaghoubi, S.S., Barrio, J.R., Namavari, M., Satyamurthy, N., Phelps, M.E., Herschman, H.R., and Gambhir, S.S., Imaging progress of herpes simplex virus type 1 thymidine kinase suicide gene therapy in living subjects with positron emission tomography. Cancer Gene Ther, 2004
16 Gambhir S.S., Barrio J.R., Herschman H.R., Phelps M.E. (1999). Imaging gene expression: principles and assays. J Nucl Cardiol.
17 Brust P., Haubner R., Friedrich A., Scheunemann M., Anton M., Koufaki O.N., Hauses M., Noll S., Noll B., Haberkorn U., Schackert G., Schackert H.K., Avril N., Johannsen B. (2001). Comparison of [18F]FHPG and [124/125I]FIAU for imaging herpes simplex virus type 1 thymidine kinase gene expression. Eur J Nucl Med.
18 Haubner R., Avril N., Hantzopoulos P.A., Gansbacher B., Schwaiger M. (2000). In vivo imaging of herpes simplex virus type 1 thymidine kinase gene expression: early kinetics of radiolabelled FIAU. Eur J Nucl Med.
19 Jacobs A., Braunlich I., Graf R., Lercher M., Sakaki T., Voges J., Hesselmann V., Brandau W., Wienhard K., Heiss W.D. (2001). Quantitative kinetics of [124I]FIAU in cat and man. J Nucl Med.
20 Tjuvajev J.G., Doubrovin M., Akhurst T., Cai S., Balatoni J., Alauddin M.M., Finn R., Bornmann W., Thaler H., Conti P.S., Blasberg R.G. (2002). Comparison of radiolabeled nucleoside probes (FIAU, FHBG, and FHPG) for PET imaging of HSV1-tk gene expression. J Nucl Med.
21 Deng W.P., Yang W.K., Lai W.F., Liu R.S., Hwang J.J., Yang D.M., Fu Y.K., Wang H.E. (2004). Non-invasive in vivo imaging with radiolabelled FIAU for monitoring cancer gene therapy using herpes simplex virus type 1 thymidine kinase and ganciclovir. Eur J Nucl Med Mol Imaging.
22 Vaidyanathan G., Zalutsky M.R. (1998). Preparation of 5-[131I]iodo- and 5-[211At]astato-1-(2-deoxy-2-fluoro-beta-D-arabinofuranosyl) uracil by a halodestannylation reaction. Nucl Med Biol.
23 Tjuvajev J.G., Finn R., Watanabe K., Joshi R., Oku T., Kennedy J., Beattie B., Koutcher J., Larson S., Blasberg R.G. (1996). Noninvasive imaging of herpes virus thymidine kinase gene transfer and expression: a potential method for monitoring clinical gene therapy. Cancer Res.
24 Miyagawa M., Anton M., Haubner R., Simoes M.V., Stadele C., Erhardt W., Reder S., Lehner T., Wagner B., Noll S., Noll B., Grote M., Gambhir S.S., Gansbacher B., Schwaiger M., Bengel F.M. (2004). PET of cardiac transgene expression: comparison of 2 approaches based on herpesviral thymidine kinase reporter gene. J Nucl Med.
25 Hackman T., Doubrovin M., Balatoni J., Beresten T., Ponomarev V., Beattie B., Finn R., Bornmann W., Blasberg R., Tjuvajev J.G. (2002). Imaging expression of cytosine deaminase-herpes virus thymidine kinase fusion gene (CD/TK) expression with [124I]FIAU and PET. Mol Imaging.
26 Jacobs A., Dubrovin M., Hewett J., Sena-Esteves M., Tan C.W., Slack M., Sadelain M., Breakefield X.O., Tjuvajev J.G. (1999). Functional coexpression of HSV-1 thymidine kinase and green fluorescent protein: implications for noninvasive imaging of transgene expression. Neoplasia.
27 Tjuvajev J.G., Joshi A., Callegari J., Lindsley L., Joshi R., Balatoni J., Finn R., Larson S.M., Sadelain M., Blasberg R.G. (1999). A general approach to the non-invasive imaging of transgenes using cis-linked herpes simplex virus thymidine kinase. Neoplasia.
28 Wen B., Burgman P., Zanzonico P., O'Donoghue J., Cai S., Finn R., Serganova I., Blasberg R., Gelovani J., Li G.C., Ling C.C. (2004). A preclinical model for noninvasive imaging of hypoxia-induced gene expression; comparison with an exogenous marker of tumor hypoxia. Eur J Nucl Med Mol Imaging.
29 Bettegowda, C., Foss, C.A., Cheong, I., Wang, Y., Diaz, L., Agrawal, N., Fox, J., Dick, J., Dang, L.H., Zhou, S., Kinzler, K.W., Vogelstein, B., and Pomper, M.G., Imaging bacterial infections with radiolabeled 1-(2'deoxy-2'-fluoro-{beta}-D-arabinofuranosyl)-5-iodouracil. Proc Natl Acad Sci U S A, 2005
30 Soghomonyan S.A., Doubrovin M., Pike J., Luo X., Ittensohn M., Runyan J.D., Balatoni J., Finn R., Tjuvajev J.G., Blasberg R., Bermudes D. (2005). Positron emission tomography (PET) imaging of tumor-localized Salmonella expressing HSV1-TK. Cancer Gene Ther.
31 Bengel F.M., Anton M., Richter T., Simoes M.V., Haubner R., Henke J., Erhardt W., Reder S., Lehner T., Brandau W., Boekstegers P., Nekolla S.G., Gansbacher B., Schwaiger M. (2003). Noninvasive imaging of transgene expression by use of positron emission tomography in a pig model of myocardial gene transfer. Circulation.
32 Jacobs A., Voges J., Reszka R., Lercher M., Gossmann A., Kracht L., Kaestle C., Wagner R., Wienhard K., Heiss W.D. (2001). Positron-emission tomography of vector-mediated gene expression in gene therapy for gliomas. Lancet.